# N-[2-[N-Ethyl-N-[2-(2-[^18^F]fluoropyridin-3-yloxy)ethyl]amino]ethyl]-6-iodoquinoxaline-2-carboxamide

Chemical name: | N-[2-[N-Ethyl-N-[2-(2-[^18^F]fluoropyridin-3-yloxy)ethyl]amino]ethyl]-6-iodoquinoxaline-2-carboxamide | [image]
Abbreviated name: | [^18^F]44 | [image]
Synonym: | | [image]
Agent Category: | Compounds | [image]
Target: | Melanin | [image]
Target Category: | Others | [image]
Method of detection: | Positron emission tomography | [image]
Source of signal / contrast: | ^18^F | [image]
Activation: | No | [image]
Studies: | - In vitro; - Rodents | Chemical structure of [^18^F]44 (1).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=benzamide+and+imaging+and+therapy)]

N-[2-[N-Ethyl-N-[2-(2-[^18^F]fluoropyridin-3-yloxy)ethyl]amino]ethyl]-6-iodoquinoxaline-2-carboxamide, abbreviated as [^18^F]44, is a quinoxaline benzamide (BZA) derivative that was synthesized for melanin-targeted radionuclide imaging and therapy of melanoma (1).

BZA derivatives represent a versatile class of aromatic compounds that possess a common structure element of Ph-CONH(CH_2_)_m_NR_2_ (m = 1, 2) and exhibit comparable properties, including high and specific binding with melanin in melanoma cells and melanocytes (2-4). Some of these compounds, such as N-(2-diethylaminoethyl)-4-[^123^I]iodobenzamide ([^123^I]BZA) and [^123^I]-N-(2-diethylaminoethyl)-2-iodobenzamide ([^123^I]BZA2), have been successfully evaluated in melanoma patients, showing high sensitivity and selectivity in the detection of melanoma and its metastasis (5-8).

The promising results with [^123^I]BZA have prompted great efforts from several groups in screening BZA analogs (2, 9, 10). Among them is a group of investigators in France who synthesized a series of BZA derivatives via structure-activity studies (11, 12). On the basis of the structure of the lead agent [^123^I]BZA, they synthesized a group of spermidine BZA derivatives by replacing the diethylaminoethyl moiety in the BZA structure with a triamine (spermidine). Spermidine BZA derivatives exhibit high affinity for melanin comparable to that of [^123^I]BZA; however, these compounds exhibit less accumulation in tumors than [^123^I]BZA in animal models of melanoma (13). More recently, the investigators generated a class of heteroaromatic BZA analogs by incorporating the heteroaromatic structure in place of the benzene moiety to take advantage of the polycyclic aromatic compounds that display a strong affinity for melanin while keeping the lipophilic side chain (14). The heteroaromatic analogs, [^125^I]5a through [^125^I]5I, showed high specific and long-lasting uptake in the melanoma, which is favorable for combined imaging and therapy. At the same time, the investigators also identified a group of quinoxaline analogs; radioiodinated derivative 3 (ICF01012) is one of these compounds, which show the most favorable pharmacokinetic properties for radionuclide therapy (15, 16). The rapid and specific tumor uptake of quinoxaline compounds also suggests that they are potentially valuable for radionuclide imaging. For radiofluorination, ICF01012 was modified by incorporating 2- or 6-fluoropyridine in the N,N-diethylethylenediamine framework of ICF01012. This strategy allows nucleophilic heteroaromatic radiofluorination of corresponding halogeno- or nitro-precursors without the need for an additional electron-withdrawing substituent in the aromatic ring. Fluoropyridine was introduced on the tertiary amine either directly or in combination with various linkers, which resulted in a group of amide tracers, such as agents [^125^I]56 and [^18^F]44 (compound 56 is the dihydrochloride salt of 44) (1). These derivatives showed favorable properties for combined radionuclide imaging (^18^F, ^125^I) and therapy (^131^I) of melanoma using a single chemical structure. The following is a list of some representative agents that were synthesized and tested by the investigators from the group in France.

BZA derivatives: [^125/123^I]BZA, [^125^I]BZA2, [^125^I]BZ18, and [^125^I]5a through [^125^I]5I; and quinoxaline derivatives: [^125/131^I]ICF01012 (or [^125/131^I]3), [^125^I]56, and [^18^F]44.

This chapter summarizes the data of imaging studies obtained with [^18^F]44 (1).

### Related Resource Links:

Melanin-targeted imaging agents in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=melanin+AND+micad%5bbook%5d&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books)

Benzamide derivatives in PubChem (http://www.ncbi.nlm.nih.gov/sites/entrez?db=pcsubstance&term=benzamide) Benzamide derivatives in clinical trials in ClinicalTrials.gov (http://clinicaltrials.gov/ct2/results?term=benzamide)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/21417462)]

Maisonial et al. prepared [^18^F]44 via a three-step, two-pot, radiosynthetic procedure that was automated with a Zymate laboratory automation system. ^18^F was incorporated into precursor 75 (tert-butyl N-[2-[N-ethyl-N-[2-(2-nitropyridin-3-yloxy)ethyl]amino]ethyl]carbamate) to give [^18^F]74 in yields ranging from 20% to 40%; acidic N-boc deprotection of [^18^F]74 generated the radioactive intermediate [^18^F]29, and acylation of [^18^F]29 to provide [^18^F]44 (1). Acylation yields of the conversion of [^18^F]29 to [^18^F]44 ranged between 20% and 40% (nonisolated decay-corrected yields). The chemical purity was >95%. [^18^F]44 could be produced in 6% to 10% nonisolated decay-corrected yields with a specific radioactivity of 0.25–0.34 TBq/μmol (6.76–9.19 Ci/µmol) (calculated from three consecutive high-performance liquid chromatography analyses) in 110−130 min.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/21417462)]

The in vitro data of the lead compound 3 were summarized in the literature regarding [^125^I]ICF01012 (or [^125^I]3) (15, 16). In vitro studies with cells were not performed for the compound 56 or the agent [^18^F]44.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/21417462)]

Positron emission tomography (PET) imaging with [^18^F]44 (7.4 MBq (0.2 mCi)) was performed in C57Bl6 mice bearing B16F0 and B16F10 tumors (n = 4). B16F0 tumors show a very high concentration of melanin, whereas B16F10 tumors exhibit a lower melanin content. Animals were imaged for up to 4 h. The peak uptake in tumors was reached ~2 h after injection, with a value of 8.3 ± 1.7% of the injected dose per volume of tissue (% ID/cc) for the B16F0 tumors and 2.1 ± 0.4% ID/cc for the B16F10 tumors. At 4 h, the values remained similar, whereas the muscle uptake dropped from 0.6 ± 0.2% ID/cc at 2 h to 0.2 ± 0.1% ID/cc at 4 h, providing a good contrast with surrounding tissues. In vitro assays to determine the tumor melanin content produced a B16F0/B16F10 ratio of ~5 (data not shown), and PET quantification of the uptake gave a ratio of 4.0 ± 0.6. The difference of melanin content is clearly reflected in the difference of uptake between the two tumors. The biodistribution and kinetics profile were consistent with those observed with [^125^I]56 (the dihydrochloride salt of 44). Blocking studies were not performed.

In summary, Maisonial et al. synthesized 14 new iodinated and fluorinated analogs of the lead compound 3 ([^131^I]3) (1). All of these tracers contain a 2- or 6-fluoropyridine moiety incorporated in the N,N-diethylethylenediamine scaffold. Most of these novel radioiodinated compounds showed significant tumor retention, especially the derivative [^125/131^I]56, which presented high, specific, and long-lasting tumor uptake combined with a rapid clearance from nontarget organs, offering both diagnostic (^125^I and ^18^F) and therapeutic (^131^I) potentialities (1).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No references are currently available.

## References

1 Maisonial A., Kuhnast B., Papon J., Boisgard R., Bayle M., Vidal A., Auzeloux P., Rbah L., Bonnet-Duquennoy M., Miot-Noirault E., Galmier M.J., Borel M., Askienazy S., Dolle F., Tavitian B., Madelmont J.C., Moins N., Chezal J.M. (2011). Single photon emission computed tomography/positron emission tomography imaging and targeted radionuclide therapy of melanoma: new multimodal fluorinated and iodinated radiotracers. J Med Chem.
2 Oltmanns D., Eisenhut M., Mier W., Haberkorn U. (2009). Benzamides as melanotropic carriers for radioisotopes, metals, cytotoxic agents and as enzyme inhibitors. Curr Med Chem.
3 Chehade F., De Labriolle-Vaylet C., Michelot J., Moins N., Moreau M.F., Hindie E., Papon J., Escaig F., Galle P., Veyre A. (2001). Distribution of I-BZA (N-2-diethylaminoethyl-4-iodobenzamide) in grafted melanoma and normal skin: a study by secondary ion mass spectroscopy. Cell Mol Biol (Noisy-le-grand).
4 Greguric I., Taylor S.R., Denoyer D., Ballantyne P., Berghofer P., Roselt P., Pham T.Q., Mattner F., Bourdier T., Neels O.C., Dorow D.S., Loc'h C., Hicks R.J., Katsifis A. (2009). Discovery of [18F]N-(2-(diethylamino)ethyl)-6-fluoronicotinamide: a melanoma positron emission tomography imaging radiotracer with high tumor to body contrast ratio and rapid renal clearance. J Med Chem.
5 Bacin F., Michelot J., Bonafous J., Veyre A., Moreau M.F., Kemeny J.L., Chossat F., Bekhechi D. (1998). Clinical study of [123I] N-(2-diethylaminoethyl)-4-iodobenzamide in the diagnosis of primary and metastatic ocular melanoma. Acta Ophthalmol Scand.
6 Michelot J.M., Moreau M.F., Veyre A.J., Bonafous J.F., Bacin F.J., Madelmont J.C., Bussiere F., Souteyrand P.A., Mauclaire L.P., Chossat F.M., et al. (1993). Phase II scintigraphic clinical trial of malignant melanoma and metastases with iodine-123-N-(2-diethylaminoethyl 4-iodobenzamide). J Nucl Med.
7 Mansard S., Papon J., Moreau M.F., Miot-Noirault E., Labarre P., Bayle M., Veyre A., Madelmont J.C., Moins N. (2005). Uptake in melanoma cells of N-(2-diethylaminoethyl)-2-iodobenzamide (BZA2), an imaging agent for melanoma staging: relation to pigmentation. Nucl Med Biol.
8 Moins N., D'Incan M., Bonafous J., Bacin F., Labarre P., Moreau M.F., Mestas D., Noirault E., Chossat F., Berthommier E., Papon J., Bayle M., Souteyrand P., Madelmont J.C., Veyre A. (2002). 123I-N-(2-diethylaminoethyl)-2-iodobenzamide: a potential imaging agent for cutaneous melanoma staging. Eur J Nucl Med Mol Imaging.
9 Labarre P., Papon J., Moreau M.F., Moins N., Bayle M., Veyre A., Madelmont J.C. (2002). Melanin affinity of N-(2-diethylaminoethyl)-4-iodobenzamide, an effective melanoma imaging agent. Melanoma Res.
10 Moins N., Papon J., Seguin H., Gardette D., Moreau M.F., Labarre P., Bayle M., Michelot J., Gramain J.C., Madelmont J.C., Veyre A. (2001). Synthesis, characterization and comparative biodistribution study of a new series of p-iodine-125 benzamides as potential melanoma imaging agents. Nucl Med Biol.
11 Desbois N., Gardette M., Papon J., Labarre P., Maisonial A., Auzeloux P., Lartigue C., Bouchon B., Debiton E., Blache Y., Chavignon O., Teulade J.C., Maublant J., Madelmont J.C., Moins N., Chezal J.M. (2008). Design, synthesis and preliminary biological evaluation of acridine compounds as potential agents for a combined targeted chemo-radionuclide therapy approach to melanoma. Bioorg Med Chem.
12 Labarre P., Papon J., Rose A.H., Guerquin-Kern J.L., Morandeau L., Wu T.D., Moreau M.F., Bayle M., Chezal J.M., Croisy A., Madelmont J.C., Turner H., Moins N. (2008). Melanoma affinity in mice and immunosuppressed sheep of [(125)I]N-(4-dipropylaminobutyl)-4-iodobenzamide, a new targeting agent. Nucl Med Biol.
13 Moreau M.F., Papon J., Labarre P., Moins N., Borel M., Bayle M., Bouchon B., Madelmont J.C. (2005). Synthesis, in vitro binding and biodistribution in B16 melanoma-bearing mice of new iodine-125 spermidine benzamide derivatives. Nucl Med Biol.
14 Chezal J.M., Papon J., Labarre P., Lartigue C., Galmier M.J., Decombat C., Chavignon O., Maublant J., Teulade J.C., Madelmont J.C., Moins N. (2008). Evaluation of radiolabeled (hetero)aromatic analogues of N-(2-diethylaminoethyl)-4-iodobenzamide for imaging and targeted radionuclide therapy of melanoma. J Med Chem.
15 Bonnet M., Mishellany F., Papon J., Cayre A., Penault-Llorca F., Madelmont J.C., Miot-Noirault E., Chezal J.M., Moins N. (2010). Anti-melanoma efficacy of internal radionuclide therapy in relation to melanin target distribution. Pigment Cell Melanoma Res.
16 Bonnet-Duquennoy M., Papon J., Mishellany F., Labarre P., Guerquin-Kern J.L., Wu T.D., Gardette M., Maublant J., Penault-Llorca F., Miot-Noirault E., Cayre A., Madelmont J.C., Chezal J.M., Moins N. (2009). Targeted radionuclide therapy of melanoma: anti-tumoural efficacy studies of a new 131I labelled potential agent. Int J Cancer.